# ^68^Ga-Trastuzumab F(ab’) fragment

Chemical name: | ^68^Ga-Trastuzumab F(ab’) fragment
Abbreviated name:
Synonym: | ^68^Ga-DCHF
Agent Category: | Trastuzumab F(ab’) fragment
Target: | Human epidermal growth factor receptor
Target Category: | Binding
Method of detection: | PET
Source of signal: | ^68^Ga
Activation: | No activation required
Studies: | - In vitro; - Rodents | View human EGFR protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=63101670) and nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucgss&id=66889325) sequence information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga-Herceptin%20F%28ab%27%29%20fragment)]

The epidermal growth factor (EGF) and its receptor (EGFR) are known to play a role in the oncogenic transformation of cells (1). The EGFR is a tyrosine kinase receptor that includes four members, EGFR and three other human EGF receptors (HERs) designated as HER2/ErbB2, HER3/ErbB3, and HER4/ErbB4. The four receptors constitute the HER-kinase axis and regulate cellular responses through complex receptor-ligand interactions. The various signal transduction pathways used by the EGFRs to mediate cell responses have been described by Brandt et al. (2). The various EGFRs are known to be amplified, mutated, or overexpressed in several cancers and are a target for the development of pharmaceutical agents that inhibit the receptor or the signal transduction pathway (3). For this inhibition, a variety of small molecules and antibodies against the EGFRs have been developed (4). However, to achieve therapeutic effects the receptor or signal transduction pathway must be involved in maintenance of the malignant phenotype because HER inhibitor therapy does not necessarily result in treatment of a cancer (5).

The use of antibodies alone against EGFR (e.g., Erbitux; cetuximab) and HER2 (Herceptin; trastuzumab) for the treatment of cancer gave only moderate results; antibodies are most useful when used in combination with chemotherapy (6, 7). Geldanamycin, an ansamycin antibiotic, has a unique mechanism for inhibition of HER2 activity by inducing protesomal degradation of the receptor. The antibiotic binds to heat shock protein 90 (Hsp90), a chaperone protein that is responsible for the maturation and stability of a variety of proteins including HER2 (8). The binding of geldanamycin to Hsp90 inhibits the maturation and stability of HER2 and leads to degradation of the receptor. The geldanamycin derivative 17-N-allylamino-17-demethoxy geldanamycin (17-AAG) was shown to exhibit antitumor activity, sensitize tumors to taxanes (drugs that inhibit cell proliferation by binding to microtubules), induce degradation of HER2, and inhibit expression of the receptor (9). This drug is being studied in several clinical trials for the treatment of various cancers (www.clinicaltrials.gov).

Because 17-AAG inhibits HER2 expression, this characteristic activity of the drug has been used to image the pharmacodynamic effects of the drug with the F(ab´) fragment of an antibody against EGFR. For this, a gallium (^68^Ga)-labeled F(ab´) fragment of trastuzumab, which is a commercially available antibody against EGFR, was used to determine the alterations of HER2 expression in response to 17-AAG (3). The ^68^Ga-labeled fragment was selected for this work because it had a 3-h half-life in serum and showed no decrease in signal even 24 h after administration.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20F%28ab%29%20herceptin%20fragment%20synthesis)]

The F(ab´) fragment of trastuzumab was generated by the digestion of trastuzumab with pepsin immobilized on agarose beads (3). Briefly, trastuzumab was diluted with sodium acetate buffer (pH 4.5) and concentrated in a centrifugal concentrator with a 60-kDa cut-off limit. This process was repeated several times and the protein was gently shaken overnight with the pepsin agarose beads. The protein fragments were obtained by removing the agarose beads after centrifugation, concentrated as before, and purified by high-performance liquid chromatography on a Superdex 200 column.

The fragments were modified with 1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) by binding one of the four carboxylic acid groups of DOTA to the primary amines in the protein structure as described by Smith-Jones et al. (10). Excess DOTA and other reactants were removed from the DOTA-F(ab´) fragment by repeated washing with sodium acetate buffer using the centrifugal concentration technique. The DOTA-conjugated trastuzumab fragment (DCHF) contained an average of 6.3 DOTA moieties per F(ab´) and were 81% immunoreactive. The fragments were labeled either with radioactive indium (^111^In) for biodistribution studies or with ^68^Ga to obtain ^68^Ga-DCHF for positron emission tomography (PET) investigations.

The radiochemical yield and specific activity of the radiochemical were not provided by the investigators; the investigators reported a linear correlation between radioactive uptake, as quantified by direct assessment of resected tumors by gamma counter, and radionuclide uptake, as estimated by PET imaging (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20F%28ab%20%29%20herceptin%20fragment%20in%20vitro)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20F%28ab%20%29%20herceptin%20fragment%20rodentia)]

The biodistribution of ^68^Ga-DCHF was used to monitor the in vivo effects of 17-AAG on HER2 expression in tumor-bearing mice using PET imaging (3). The level of HER2 expression was determined in control mice (without 17-AAG treatment) and 17-AAG–treated mice bearing BT-474 human breast cancer xenografts. The control mice showed a constant or slightly increased HER2 expression by PET imaging over a 24-h period. In contrast, animals treated with 17-AAG showed an 80% reduction in HER2 expression 24 h after treatment, but HER2 increased to 50% of the initial expression up to 7 days after treatment. During the same period the control animals showed a 20% increase in HER2 expression up to 7 days after treatment compared to the pretreatment levels.

A decrease in ^68^Ga-DCHF uptake by the tumors was observed in response to the 17-AAG treatment, although no change in distribution of the radiochemical was observed in other organs (heart, lung, liver, spleen, etc.). When the radionuclide uptake was adjusted to account for the nonspecific background, the accumulation of radioactivity by the tumors correlated well with the data obtained by immunoblotting and microPET region-of-interest analysis.

The possible use of this technique to image pharmacodynamic effects of antireceptor antibodies and tyrosine kinase and Hsp90 inhibitors was suggested (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20F%28ab%20%29%20herceptin%20fragment%20non-primate%20mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20F%28ab%20%29%20herceptin%20fragment%20non-human%20primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20F%28ab%20%29%20herceptin%20fragment%20humans)]

No publications are currently available.

## References

1 Gross M.E. Shazer R.L. Agus D.B. Targeting the HER-kinase axis in cancer Semin Oncol 2004 31 Suppl 3 1 9 20 15052539
2 Brandt B., Meyer-Staeckling S., Schmidt H., Agelopoulos K., Buerger H. (2006). Mechanisms of egfr gene transcription modulation: relationship to cancer risk and therapy response. Clin Cancer Res.
3 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
4 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
5 Bates S.E., Fojo T. (2005). Epidermal growth factor receptor inhibitors: a moving target?. Clin Cancer Res.
6 Khalil M.Y., Grandis J.R., Shin D.M. (2003). Targeting epidermal growth factor receptor: novel therapeutics in the management of cancer. Expert Rev Anticancer Ther.
7 Sledge G.W. Gemcitabine combined with paclitaxel or paclitaxel/trastuzumab in metastatic breast cancer Semin Oncol 2003 30 Suppl 3 2 19 21 12722021
8 Neckers L. Hsp90 inhibitors as novel cancer chemotherapeutic agents Trends Mol Med 2002 8 4 Suppl S55 61 11927289
9 Solit D.B., Basso A.D., Olshen A.B., Scher H.I., Rosen N. (2003). Inhibition of heat shock protein 90 function down-regulates Akt kinase and sensitizes tumors to Taxol. Cancer Res.
10 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.